# (S)-1-(4–2-[^11^C]Methoxybenzyl)-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione

Chemical name: | (S)-1-(4–2-[^11^C]Methoxybenzyl)-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione
Abbreviated name: | [^11^C]WC-98
Synonym:
Agent category: | Compound
Target: | Caspase-3
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=WC-II-89)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene-regulated (2) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes called caspases and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced in particular by epithelial cells from many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathological conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^18^F, ^123^I, ^125^I, and ^99m^Tc for imaging (9-12). However, annexin V is not able to distinguish between apoptosis and necrosis. However, PS is expressed in both cell necrosis and apoptosis and therefore cannot distinguish between the two, whereas caspase 3/7 is only activated in apoptosis. Caspase substrate may be an attractive alternative for imaging cells undergoing apoptosis because caspases are key enzymes that mediate apoptosis (13). Chu et al. (14) reported that isatin sulfonamide analogs exhibited selective inhibition of caspase-3 and caspase-7 (executioner caspases) over caspase-1, -6, and -8 (initiator caspases). 1-[4-(2-[^18^F]Fluoroethoxy)-benzyl]-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione ([^18^F]WC-II-89) showed higher uptake in the liver and spleen in cycloheximide-treated rats when compared with untreated control rats (15). (S)-1-(4–2-[^11^C]Methoxybenzyl)-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione ([^11^C]WC-98), an analog of [^18^F]WC-II-89, has been synthesized for imaging caspase-3 activation in apoptosis (16).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20synthesis)]

Zhou et al. (16) reported the synthesis of [^11^C]WC-98 in one-pot reactions. (S)-1-(4-Hydroxybenzyl)-5-(2-phenoxymethyl-pyrrolidine-1-sulfonyl)-1H-indole-2,3-dione (410 nM) was added to a solution of 1 M Bu_4_NOH (830 nM) in CH_3_CN. After cooling to 0ºC, [^11^C]CH_3_I was bubbled into the mixture and heated at 88ºC for 4 min, and then 88ºC for 4 min with 1 N HCl. [^11^C]WC-98 was purified with high-performance liquid chromatography. The radiochemical yield was 62 ± 12% (n = 4) at the end of purification, and the specific activity was 207.2 ± 40.7 GBq/µmol (5.6 ± 1.1 Ci/µmol) at the end of synthesis (EOS). Radiochemical purity was >99% as determined with high-performance liquid chromatography. Total synthesis time was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+WC-II-89+and+in+vitro)]

In vitro caspase enzyme assays using WC-II-89 showed inhibition concentration (IC_50_) values of 9.7 ± 1.3 nM for caspase-3, 23.5 ± 3.5 nM for caspase-7, 3,700 ± 390 nM for caspase-6, >50,000 nM for caspase-1, and >50,000 nM for caspase-8 (15).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20rodentia)]

Zhou et al. (16) performed ex vivo liver accumulation of [^11^C]WC-98 in normal mice and mice pretreated with anti-Fas (Jo2) antibody to induce apoptosis in the liver (n = 5/group). The initial tracer accumulation (~25%ID/g) was similar in the liver from both mice at 5 min after injection. However, the Fas-treated liver (~13% ID/g) showed a higher retention of radioactivity than the control liver (~2% ID/g) at 30 min after injection. Fluorometric caspase-3 enzymatic assay confirmed a 5-fold increase in the Fas-treated liver over the control livers. The microPET imaging confirmed the approximately 5-fold increase in [^11^C]WC-98 accumulation in the Fas-treated liver at 30 min after injection as observed in the biodistribution study. The Fas-treated liver (~0.12% ID/ml) was still clearly visualized at 30-60 min, whereas the control liver (~0.02% ID/ml) was barely visualized. No blocking or caspase-3 inhibition experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20WC-II-89%20and%20human)]

No publications are currently available.

## NIH Support

P01 HL13851, K08 EB006702, R21 CA121952

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
12 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
13 Neuss M., Crow M.T., Chesley A., Lakatta E.G. (2001). Apoptosis in cardiac disease--what is it--how does it occur. Cardiovasc Drugs Ther.
14 Chu W., Zhang J., Zeng C., Rothfuss J., Tu Z., Chu Y., Reichert D.E., Welch M.J., Mach R.H. (2005). N-benzylisatin sulfonamide analogues as potent caspase-3 inhibitors: synthesis, in vitro activity, and molecular modeling studies. J Med Chem.
15 Zhou D., Chu W., Rothfuss J., Zeng C., Xu J., Jones L., Welch M.J., Mach R.H. (2006). Synthesis, radiolabeling, and in vivo evaluation of an 18F-labeled isatin analog for imaging caspase-3 activation in apoptosis. Bioorg Med Chem Lett.
16 Zhou D., Chu W., Chen D.L., Wang Q., Reichert D.E., Rothfuss J., D'Avignon A., Welch M.J., Mach R.H. (2009). [18F]- and [11C]-labeled N-benzyl-isatin sulfonamide analogues as PET tracers for apoptosis: synthesis, radiolabeling mechanism, and in vivo imaging study of apoptosis in Fas-treated mice using [11C]WC-98. Org Biomol Chem.